# Quantum dot800-poly(ethylene glycol)-c(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | Quantum dot800-poly(ethylene glycol)-c(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | QD800-RGD, QD800-PEG-c(RGDyK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Quantum dot
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1–10 nm (6-8). They can be tuned to emit signals in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow, symmetric emission spectra with long, excited-state lifetimes (20–50 ns) compared with those of fluorescent dyes (1–10 ns). They process good quantum yields of 40%–90% and possess high extinction coefficients. They are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which have been tested in vitro and in vivo (8-12). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are limited studies of long-term toxicity of QDs in small animals (13-21); little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans. The performance of various nanoparticles for biomedical imaging has been reviewed (22, 23).

Integrins are a family of heterodimeric, cell-surface glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (24). Integrins comprise an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class, affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (25-30). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and on most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (29, 31, 32). A tripeptide sequence comprising Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled cyclic RGD peptides have been introduced for tumor imaging and tumor angiogenesis (33).

QDs that do not contain Cd (non-Cd QDs) have been prepared as an alternative to the more toxic Cd-based QDs. These newly developed non-Cd QDs exhibit improved blood half-life and minimal reticuloendothelial system accumulation with rapid renal clearance (34). These QDs easily extravasate leaky tumor blood vessels because of their enhanced permeability and retention effects. Gao et al. (35) coated non-Cd QD800 (InAs/InP/ZnSe, emission maximum at 800 nm) with di-stearoyl-poly(ethylene glycol)-phosphatidylethanolamine 2000 (DSPE-PEG2000) and c(RGDyK) to form QD800-PEG-RGD for NIR fluorescence imaging of α_v_β_3_ integrin expression in the tumor vasculature in mice. QD800-PEG-RGD has been shown to have a high accumulation in tumors with little extravasation and a predominant liver accumulation.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+synthesis)]

QD800 (10 nmol In) and DSPE-PEG2000 amine (1,800 nmol) were mixed in chloroform (35). Water was added upon complete removal of chloroform at room temperature. QD800-PEG was purified with centrifugation to remove excess DSPE-PEG2000 amine. A solution of QD800-PEG (1 nmol) and 4-maleimidobutyric acid N-hydroxysuccinimide ester in borate buffer (pH 8.5) was incubated for 2 h at room temperature. Thiolated RGD peptide (c(RGDy(ε-acetylthiol)K) (1 µmol) and the activated QD800-PEG sample were incubated for 2 h at room temperature. The product, QD800-PEG-RGD, was purified with column chromatography. QD800-PEG-RAD was similarly prepared as a negative control using c(RADy(ε-acetylthiol)K. The conjugation efficiency was 40%–50%. QD800-PEG-RGD, QD800-PEG-RAD, and QD800-PEG had hydrodynamic diameters of 19.6 nm, 20.1 nm, and 16.5 nm, respectively, in phosphate-buffered saline (PBS) as measured with dynamic light scattering. There were 20–35 peptides per QD.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+in%20vitro)]

Gao et al. (35) showed that QD800-PEG-RGD, QD800-PEG-RAD, and QD800-PEG maintained their optical properties with an emission maximum at ~800 nm in PBS or 90% mouse serum. More than 80% of the emission intensity of QD800-PEG-RGD and QD800-PEG-RAD remained in mouse serum after incubation for 24 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+rodentia)]

Gao et al. (35) used a whole-body NIR fluorescence imaging system at 0.5, 1, 4, 5, 6, 18, and 24 h after QD injection to study the accumulation of QD800-PEG-RGD, QD800-PEG-RAD, and QD800-PEG in mice bearing U87MG tumors. The QDs (200 nmol/mouse) were injected intravenously into the tumor-bearing nude mice (n = 3/group). QD800-PEG-RGD showed good NIR fluorescence intensity and contrast in the tumors as early as 0.5 h after injection. Tumor signal increased with QD800-PEG-RGD to a maximum by 1 h and then gradually decreased. The tumor/background ratios with QD800-PEG-RGD were 3.26, 4.26, 3.46, 2.90, 2.85, 2.04, and 1.83 at 0.5, 1, 4, 5, 6, 18, and 24 h after injection, respectively. On the other hand, QD800-PEG-RAD and QD800-PEG showed little tumor contrast. The maximum tumor/background ratio with these agents was ~2 for QD800-PEG-RAD at 0.5 h, and this ratio decreased to ~1 at 18 h. The tumor/background ratios for QD800-PEG were ~1 at all the time points. Bright NIR fluorescence was observed in the liver, spleen, and bone marrow for all three QDs. Ex vivo NIR fluorescence imaging scans were performed on tissues harvested at 4 h. The tumor accumulation was 10.7 ± 1.5% injected dose/gram (ID/g), 4.0 ± 0.5% ID/g, and 2.9 ± 0.3% ID/g for QD800-PEG-RGD, QD800-PEG-RAD, and QD800-PEG, respectively. The liver (50%–60% ID/g), lung (~10% ID/g), and spleen (~10% ID/g) all had strong signals, and the U87MG tumor exhibited higher uptake than the heart, kidneys, intestine, bone, and muscle. Immunostaining of tumor sections showed that QD800-PEG-RGD bound to the endothelial cells and did not extravasate the tumor vessels. In another imaging experiment using LS174T tumor (low expression of α_v_β_3_), accumulation of QD800-PEG-RGD in the tumor was 2.8% ID/g. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=QD800%20RGD+human)]

No publication is currently available.

## NIH Support

R21 CA121842, U54 CA119367

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Zheng G., Li H., Yang K., Blessington D., Licha K., Lund-Katz S., Chance B., Glickson J.D. (2002). Tricarbocyanine cholesteryl laurates labeled LDL: new near infrared fluorescent probes (NIRFs) for monitoring tumors and gene therapy of familial hypercholesterolemia. Bioorg Med Chem Lett.
7 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
8 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
9 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
10 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
11 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
12 Kabas J.S., Kisslo J., Flick C.L., Johnson S.H., Craig D.M., Stanley T.E., Smith P.K. (1990). Intraoperative perfusion contrast echocardiography. Initial experience during coronary artery bypass grafting. J Thorac Cardiovasc Surg.
13 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
14 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
15 Kim S., Lim Y.T., Soltesz E.G., De Grand A.M., Lee J., Nakayama A., Parker J.A., Mihaljevic T., Laurence R.G., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V. (2004). Near-infrared fluorescent type II quantum dots for sentinel lymph node mapping. Nat Biotechnol.
16 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
17 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
18 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
19 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
20 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
21 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
22 Choi H.S., Frangioni J.V. (2010). Nanoparticles for biomedical imaging: fundamentals of clinical translation. Mol Imaging.
23 Swierczewska M., Lee S., Chen X. (2011). Inorganic nanoparticles for multimodal molecular imaging. Mol Imaging.
24 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
25 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
26 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
27 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
28 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
29 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
30 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
31 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
32 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
33 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
34 Xie R., Chen K., Chen X., Peng X. (2008). InAs/InP/ZnSe Core/Shell/Shell Quantum Dots as Near-Infrared Emitters: Bright, Narrow-Band, Non-Cadmium Containing, and Biocompatible. Nano Res.
35 Gao J., Chen K., Xie R., Xie J., Yan Y., Cheng Z., Peng X., Chen X. (2010). In vivo tumor-targeted fluorescence imaging using near-infrared non-cadmium quantum dots. Bioconjug Chem.